# Gd-DOTA-c(Cys-Arg-Gly-Asp-Cys)

Chemical name: | Gd-DOTA-c(Cys-Arg-Gly-Asp-Cys)
Abbreviated name: | P975
Synonym:
Agent category: | Peptide
Target: | Platelet glycoprotein GPIIb/IIIa receptor (CD61/CD41)
Target category: | Receptor
Method of detection: | Magnetic resonance imaging (MRI)
Source of signal: | Gd
Activation: | No
Studies: | - In vitro; - Rodents | Structure is not available in PubChem.

## Background

[PubMed (http://www.ncbi.nlm.nih.gov/sites/entrez?Db=pubmed&Cmd=DetailsSearch&Term=P975)]

Magnetic resonance imaging (MRI) maps information about tissues spatially and functionally. Protons (hydrogen nuclei) are widely used to create images because of their abundance in water molecules, which comprise >80% of most soft tissues. The contrast of proton MRI images depends mainly on the density of nuclear proton spins, the relaxation times of the nuclear magnetization (T1, longitudinal; T2, transverse), the magnetic environment of the tissues, and the blood flow to the tissues. However, insufficient contrast between normal and diseased tissues requires the use of contrast agents. Most contrast agents affect the T1 and T2 relaxation of the surrounding nuclei, mainly the protons of water. T2* is the spin–spin relaxation time composed of variations from molecular interactions and intrinsic magnetic heterogeneities of tissues in the magnetic field (1). Cross-linked iron oxide (CLIO) and other iron oxide formulations affect T2 primarily and lead to a decreased signal. On the other hand, paramagnetic T1 agents, such as gadolinium (Gd^3+^) and manganese (Mn^2+^), accelerate T1 relaxation and lead to increased contrast images.

Thrombosis plays a major role in many cardiovascular diseases, such as myocardial infarction, pulmonary embolism (PE), deep venous thrombosis (DVT), atherothrombosis, or cerebral venous thrombosis (2, 3). DVT is a significant cause of PE, which is a potentially life-threatening clinical problem. Thrombosis occurs when platelets deposit in regions of low flow in the deep venous system, followed by an activation process of thrombin, which then converts fibrinogen into fibrin. Platelets become activated and bind to fibrinogen, resulting in platelet aggregation via the platelet integrin GPIIb/IIIa (α_IIb_β_3_, CD61/CD41). The thrombus may become organized or detached from the vessel wall.

A single-chain antibody (anti-LIBS 145) has been developed to recognize ligand-induced binding sites (LIBS) of GPIIb/IIIa that become exposed only upon binding to fibrinogen (4). Anti-LIBS 145 single-chain antibody does not bind to circulating platelets. Anti-LIBS 145 single-chain antibody was conjugated to microparticles of iron oxide (MPIOs) to form LIBS-MPIOs for T2-weighted MRI imaging of platelet-containing thrombi (5-8). The cyclic peptide P977 (cyclo(Cys-Arg-Gly-Asp-Cys)) was found to bind to platelet glycoprotein GPIIb/IIIa receptor with good affinity (9). P975 is composed of P977-conjugated gadolinium-tetraazacyclododecane-N,N’,N’’,N’’’-tetraacetic acid (Gd-DOTA) (10). P975 is being developed as a non-invasive T1 MRI agent for GPIIb/IIIa expression in thrombi.

### Related Resource Links:

- Chapters in MICAD (http://www.ncbi.nlm.nih.gov/sites/entrez?db=Books&cmd=Search&term=GPIIb/IIIa%20+AND+micad%5bbook%5d&doptcmdl=TOCView&log%24=booksrch&bname=micad)
- Gene information in NCBI (GPIIIa/CD61 (http://www.ncbi.nlm.nih.gov/gene/3690), GPIIb/CD41 (http://www.ncbi.nlm.nih.gov/gene/3674))
- Articles in OMIM (http://www.ncbi.nlm.nih.gov/omim/?term=VCAM-1) (GPIIIa/CD61 (http://www.ncbi.nlm.nih.gov/entrez/dispomim.cgi?id=173470), GPIIb/CD41 (http://www.ncbi.nlm.nih.gov/entrez/dispomim.cgi?id=607759))
- Clinical trials (Integrin (http://www.clinicaltrials.gov/ct2/results?term=integrin))
- Drug information in FDA (http://google2.fda.gov/search?q=integrin&client=FDAgov&site=FDAgov&lr=&proxystylesheet=FDAgov&output=xml_no_dtd&getfields=*&x=17&y=16)

## Synthesis

[PubMed (http://www.ncbi.nlm.nih.gov/sites/entrez?Db=pubmed&Cmd=DetailsSearch&Term=P975+and+synthesis)]

Gd-DOTA was conjugated to P977 via a small linker at a 1:1 ratio (10). P975 exhibited an r_1_ relaxivity value of 9 mM^-1^s^-1^ at 40°C and 60 MHz.

## In Vitro Studies: Testing in Cells and Tissues

[PubMed (http://www.ncbi.nlm.nih.gov/sites/entrez?Db=pubmed&Cmd=DetailsSearch&Term=P975+and+in+vitro)]

In vitro competition binding to activated platelets was performed using FITC-fibrinogen with P975 and P977 (10). The 50% inhibition concentrations for P975 and P977 were 2.1 ± 0.3 µM and 1.6 ± 0.2 µM, respectively.

## Animal Studies

### Rodents

[PubMed (http://www.ncbi.nlm.nih.gov/sites/entrez?Db=pubmed&Cmd=DetailsSearch&Term=P975+and+rodentia)]

Klink et al. (10) performed in vivo T1-weighted MRI (9.4 T) of arachidonic acid–treated right carotid arteries in mice (n = 5/group) to induce thrombosis. P975 or Gd-DOTA (0.1 mmol/kg) was injected intravenously after thrombus formation. MRI scans were performed every 15 min up to 120 min after injection. An initial signal enhancement was observed with both P975 and Gd-DOTA in the lumen of the thrombosed carotid artery at 30 min after injection. However, there was a rapid washout with Gd-DOTA. The enhancement with P975 persisted over time and was still present at 120 min. There were three-fold, six-fold, and seven-fold increases in change in contrast/noise ratio for the P975 group compared with the Gd-DOTA group, the sham surgery group, and the control group (P < 0.01), respectively, at 120 min after injection. Injection of eptifibatide (GPIIb/IIIa antagonist) a few minutes before injection of P975 reduced the signal enhancement in the P975 group to the level of the Gd-DOTA group at 120 min after injection.

### Other Non-Primate Mammals

[PubMed (http://www.ncbi.nlm.nih.gov/sites/entrez?Db=pubmed&Cmd=DetailsSearch&Term=P975+and+(dog+or+sheep+or+pig+or+rabbit))]

No publication is currently available.

### Non-Human Primates

[PubMed (http://www.ncbi.nlm.nih.gov/sites/entrez?Db=pubmed&Cmd=DetailsSearch&Term=P975+and+(primate+not+human))]

No publication is currently available.

## Human Studies

[PubMed (http://www.ncbi.nlm.nih.gov/sites/entrez?Db=pubmed&Cmd=DetailsSearch&Term=P975+and+human)]

No publication is currently available.

## NIH Support

R01 HL71021, R01 HL78667, R01 EB009638

## References

1 Wang Y.X., Hussain S.M., Krestin G.P. (2001). Superparamagnetic iron oxide contrast agents: physicochemical characteristics and applications in MR imaging. Eur Radiol.
2 Corti R., Fuster V. (2003). New understanding, diagnosis, and prognosis of atherothrombosis and the role of imaging. Am J Cardiol.
3 Taillefer R. (2001). Radiolabeled peptides in the detection of deep venous thrombosis. Semin Nucl Med.
4 Schwarz M., Katagiri Y., Kotani M., Bassler N., Loeffler C., Bode C., Peter K. (2004). Reversibility versus persistence of GPIIb/IIIa blocker-induced conformational change of GPIIb/IIIa (alphaIIbbeta3, CD41/CD61). J Pharmacol Exp Ther.
5 von zur Muhlen C., Peter K., Ali Z.A., Schneider J.E., McAteer M.A., Neubauer S., Channon K.M., Bode C., Choudhury R.P. (2009). Visualization of activated platelets by targeted magnetic resonance imaging utilizing conformation-specific antibodies against glycoprotein IIb/IIIa. J Vasc Res.
6 von Zur Muhlen C., Sibson N.R., Peter K., Campbell S.J., Wilainam P., Grau G.E., Bode C., Choudhury R.P., Anthony D.C. (2008). A contrast agent recognizing activated platelets reveals murine cerebral malaria pathology undetectable by conventional MRI. J Clin Invest.
7 von Zur Muhlen C., von Elverfeldt D., Choudhury R.P., Ender J., Ahrens I., Schwarz M., Hennig J., Bode C., Peter K. (2008). Functionalized magnetic resonance contrast agent selectively binds to glycoprotein IIb/IIIa on activated human platelets under flow conditions and is detectable at clinically relevant field strengths. Mol Imaging.
8 von zur Muhlen C., von Elverfeldt D., Moeller J.A., Choudhury R.P., Paul D., Hagemeyer C.E., Olschewski M., Becker A., Neudorfer I., Bassler N., Schwarz M., Bode C., Peter K. (2008). Magnetic resonance imaging contrast agent targeted toward activated platelets allows in vivo detection of thrombosis and monitoring of thrombolysis. Circulation.
9 Yamada T., Kidera A. (1996). Tailoring echistatin to possess higher affinity for integrin alpha(IIb)beta(3). FEBS Lett.
10 Klink A., Lancelot E., Ballet S., Vucic E., Fabre J.E., Gonzalez W., Medina C., Corot C., Mulder W.J., Mallat Z., Fayad Z.A. (2010). Magnetic resonance molecular imaging of thrombosis in an arachidonic acid mouse model using an activated platelet targeted probe. Arterioscler Thromb Vasc Biol.